# 3,7-bis(dimethylamino)-phenothiazin-5-ium chloride

Chemical name: | 3,7-bis(dimethylamino)-phenothiazin-5-ium chloride
Abbreviated name: | Methylene blue
Synonym: | [7-(dimethylamino)phenothiazin-3-ylidene]-dimethylazanium chloride
Agent Category: | Compound
Target: | Methemoglobin, guanylyl cyclase (putative), monoamine oxidase (putative)
Target Category: | Non-targeted for viewing synovial lymph nodes; Heme protein for methemoglobin
Method of detection: | Ultrasound imaging (photoacoustic imaging)
Source of signal / contrast: | Methylene blue
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=photoacoustic%20imaging%20of%20cancer&cmd=DetailsSearch)]

A sentinel lymph node (SLN)is the first lymph node showing presence of metastasized cancer cells from a tumor. An SLN biopsy (SLNB) is the method of choice to stage breast cancer (i.e., to describe the stage of cancer progress using numbers I to IV, going from low to highest progression) in patients exhibiting clinically negative (i.e., without metastases) axillary lymph nodes (1, 2). Once detected and confirmed, the metastatic spread of the cancer from the primary tumor to the axillary lymph nodes through the lymphatic system is then tracked with either a radiolabeled sulfur colloid and/or a blue dye (isosulfan blue or methylene blue; neither of these dyes are approved by the United States Food and Drug Administration (FDA) for this application) (2). After visual confirmation, the SLN is surgically resected, and the definitive presence of cancer is established with histological methods. Although the SLNB procedure is minimally invasive, it has a 5%–10% false negative rate of detecting cancer and can possibly lead to lymphedema, seroma formation (collection of fluid under the skin), injury to local sensory nerves, and a reduction in the patient's range of motion (1, 2). In some cases, ultrasonography (US), which is the detection of high frequency sound waves, is used to identify a SLN, and a biopsy is obtained with a fine-needle aspiration biopsy (FNAB). The biopsy sample is then subjected to molecular analysis using the real-time reverse transcription-polymerase chain reaction to detect cancer in the tissue from the breast. A limitation of using US to identify a SLN is that it can only determine the size and shape of the lymph node but cannot specifically distinguish between a cancerous and a non-cancerous lymph node; this limitation reduces the sensitivity of the FNAB procedure to detect a malignancy (3).

Photoacoustic imaging (PAI) is a noninvasive method that does not involve the use of ionizing radiation for the detection of cancer. This technique, which uses a combination of the optical and US imaging modalities to detect malignant lesions, angiogenesis, etc (4), has been described in detail elsewhere (5). In brief, application of a pulse of light to biological tissue results in the generation of ultrasonic waves (photoacoustic waves) due to the thermoelastic expansion and contraction of the tissue (i.e., a fraction of the light is converted into heat within the tissue). Subsequently, the photoacoustic waves are captured with a suitable device (transducer) that captures the US waves and converts them into an image. If used by itself, optical imaging has a limited imaging depth and spatial resolution because light is scattered by the tissue. As a result, images generated with US alone have a low contrast and are speckled (5). The main advantage of using PAI is that the depth and resolution of an image can be improved by controlling the detection frequency of the transducer, and the quality of the images can be further enhanced by using intrinsic contrast agents (e.g., melanin and hemoglobin) or exogenous contrast agents (e.g., an organic dye such as methylene blue, nanoparticles, etc.) (5).

Methylene blue is an aromatic compound that has many applications in biology and medicine. In the laboratory, methylene blue is often used to stain blood cells for histological investigations, to detect nucleic acids on blots, and to determine the viability of yeast cells. Although methylene blue is not approved (http://dailymed.nlm.nih.gov/dailymed/drugInfo.cfm?id=22970) for clinical use by the FDA, it is available commercially (http://www.americanregent.com/documents/Product36PrescribingInformation.pdf) in the United States for off label use as an intravenous injection to treat methemoglobinemia (http://www.nlm.nih.gov/medlineplus/ency/article/000562.htm). Methylene blue is also under investigation in clinical trials (http://clinicaltrials.gov/ct2/results?term=methylene+blue&recr=Open) to treat osteoarthritis, to detect invasive aspergillosis (http://www.nlm.nih.gov/medlineplus/aspergillosis.html), and to map and localize SLN in breast and thyroid cancer patients. In several European countries, a procedure using methylene blue has been approved to reduce the pathogen load (e.g., viruses such as HIV and hepatitis B and C) in individual units of human plasma to be used for transfusion purposes (6). It has been shown that methylene blue radiolabeled with astatine-211 is suitable for the diagnosis and selective treatment of melanoma in mice (7). Investigators have also shown that methylene blue encapsulated in nanoparticles can be used for in vivo imaging and photodynamic therapy in mice (exposure of methylene blue nanoparticles to high-energy light pulses results in the production of nascent oxygen that damages the nucleic acids in the cells) (8).

Recently, in an effort to develop an alternative method to SLNB and FNAB for the detection of SLNs in breast cancer patients, methylene blue has been successfully used as a contrast agent to visualize SLN in rats with PAI (1, 2).

### Other Sources of Information

Information on FDA website (methylene blue (http://google2.fda.gov/search?q=methylene+blue&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*))

Other uses (http://www.google.com/#q=uses+of+methylene+blue&hl=en&prmd=ivnsb&source=univ&tbm=bks&tbo=u&ei=GUejTdi5B8uD0QGYg5yeBQ&sa=X&oi=book_group&ct=title&cad=bottom-3results&resnum=11&ved=0CGoQsAMwCg&bav=on.2,or.r_gc.r_pw.&fp=c2168e4b91ffc41a) of methylene blue.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=synthesis%20of%20methylene%20blue&cmd=DetailsSearch)]

The synthesis of methylene blue has been described in a patent (WO/2006/032879 (http://www.wipo.int/patentscope/search/en/detail.jsf?docId=WO2006032879&recNum=1&docAn=GB2005003634&queryString=FP:(WO/2006/032879)&maxRec=1)) available from the World Intellectual Property Organization (a specialized agency of the United Nations) (9). The dye is available in the United States as a 1% (W/V) solution (http://www.americanregent.com/documents/Product36PrescribingInformation.pdf) in water for injection.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20in%20vitro)]

In vitro kinetic assays and changes in visible spectra have shown that methylene blue is a potent reversible inhibitor of purified human monoamine oxidase (10). In a study to investigate the influence of methylene blue on rat hippocampal CA1 neurons, the dye was reported to decrease voltage-gated sodium channel currents and to modify the action potential of this tissue (11). However, it is important to mention these observations are not applicable to the visualization of SLNs because the dye appears to flow through the lymph system and does not localize in the nodes.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=methylene%20blue%20rodentia&cmd=DetailsSearch)]

The PAI system used to obtain the SLN images in rats consisted of a pulsed laser with a wavelength of 635 nm, which is close to 677 nm, the maximum absorption wavelength of methylene blue and ten-fold higher than that of 95% oxygenated hemoglobin (on a molar basis). The transducers used in conjunction with the pulsed laser had central frequencies of 3.5 and 5 MHz and focal lengths of 4.95 and 2.54 cm, respectively (1).

For the initial study, a rat was administered 0.07 ml 1% methylene blue in the left forepaw pad (1). PAI was performed on the animal immediately before and after injection. A SLN containing methylene blue was distinguished from a group of lymph nodes containing no dye as described by Song et al. (1). Without a methylene blue injection, only the vasculature around the lymph node was clearly visible with PAI (contrast 51 ± 7 compared to background). After the methylene blue treatment, the SLN was clearly visible (contrast 146 ± 41 compared to background), although the optical absorption of the blood also increased. After the administration of methylene blue, the contrast ratio between the SLN and the blood was reported to be ~2. The SLN was shown to be clearly visible for up to ~50 min after injection, even after repositioning the transducer. Similar results were obtained with PAI in another rat that had been injected with the dye. From this study, the investigators concluded that the PAI procedure was sensitive and suitable to detect methylene blue within a SLN in rodents (1).

In another study, a clinical US scanner was modified to perform PAI of SLN in rats (n = 7) injected with methylene blue as described above (2). From images obtained before and after injection in these animals, it was clear that SLN containing the dye generated strong photoacoustic signals, and the lymph nodes were visible up to 2.5 cm below the top surface of the overlying tissue. The animals were euthanized after the imaging was completed, and the presence of methylene blue in the SLN of the left axilla was confirmed with visual inspection of the lymph node. In addition, the optical spectrum of the photoacoustic signals was reported to match the optical absorption spectrum of methylene blue (R = 0.995) and confirmed the presence of the dye in the lymph nodes. The investigators concluded that this study was an important step toward the translation of PAI to the clinic for the noninvasive detection of SLNs (2).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=methylene%20blue%20Non-Primate%20Mammals&cmd=DetailsSearch)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=methylene%20blue%20Non-Human%20Primates&cmd=DetailsSearch)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=methylene%20blue%20Human%20Studies&cmd=DetailsSearch)]

No publication is currently available.

## Supplemental Information

[Disclaimers]

No information is currently available.

## NIH Support

Supported in part by National Institutes of Health grants R01 EB000712 and R01 NS46214

## References

1 Song K.H., Stein E.W., Margenthaler J.A., Wang L.V. (2008). Noninvasive photoacoustic identification of sentinel lymph nodes containing methylene blue in vivo in a rat model. J Biomed Opt.
2 Erpelding T.N., Kim C., Pramanik M., Jankovic L., Maslov K., Guo Z., Margenthaler J.A., Pashley M.D., Wang L.V. (2010). Sentinel lymph nodes in the rat: noninvasive photoacoustic and US imaging with a clinical US system. Radiology.
3 Koelliker S.L., Chung M.A., Mainiero M.B., Steinhoff M.M., Cady B. (2008). Axillary lymph nodes: US-guided fine-needle aspiration for initial staging of breast cancer--correlation with primary tumor size. Radiology.
4 Zhang H.F., Maslov K., Stoica G., Wang L.V. (2006). Functional photoacoustic microscopy for high-resolution and noninvasive in vivo imaging. Nat Biotechnol.
5 Kim C., Favazza C., Wang L.V. (2010). In vivo photoacoustic tomography of chemicals: high-resolution functional and molecular optical imaging at new depths. Chem Rev.
6 Seghatchian J., Walker W.H., Reichenberg S. (2008). Updates on pathogen inactivation of plasma using Theraflex methylene blue system. Transfus Apher Sci.
7 Link E.M., Michalowski A.S., Rosch F. (1994). 211At-methylene blue in targeted radiotherapy of disseminated melanoma. Pigment Cell Res.
8 He X., Wu X., Wang K., Shi B., Hai L. (2009). Methylene blue-encapsulated phosphonate-terminated silica nanoparticles for simultaneous in vivo imaging and photodynamic therapy. Biomaterials.
9 Storey, J.M.D., J.P. Sinclair, C. Marshall, H.W. Tan, and C.M. Wischik, Methods of chemical synthesis and purification of diaminophenothiazinium compounds including methylthioninium chloride (MTC), in World Intellectual Property Organization, IP services, Geneva, Switzerland2006, Wista Laboratories Ltd., Singapore.
10 Ramsay R.R., Dunford C., Gillman P.K. (2007). Methylene blue and serotonin toxicity: inhibition of monoamine oxidase A (MAO A) confirms a theoretical prediction. Br J Pharmacol.
11 Zhang Y., Zhao J., Zhang T., Yang Z. (2010). In vitro assessment of the effect of methylene blue on voltage-gated sodium channels and action potentials in rat hippocampal CA1 pyramidal neurons. Neurotoxicology.